# N-(2-Diethylaminoethyl)-4-[^18^F]fluorobenzamide for imaging melanoma

Chemical name: | N-(2-Diethylaminoethyl)-4-[^18^F]fluorobenzamide for imaging melanoma
Abbreviated name: | [^18^F]-DAFBA
Synonym: | ^18^F-FBZA
Agent Category: | Compounds
Target: | Melanin
Target Category: | Others
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation:
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=melanoma+and+imaging)]

Melanoma is one of the most deadly cancers in the United States. Although it accounts for only 4% of all skin cancer cases, melanoma is associated with ~79% of skin cancer–related deaths (1-3). The prognosis and the patient’s survival depend heavily on the clinical stage of the disease (http://www.cancer.gov/cancertopics/pdq/treatment/melanoma/HealthProfessional/page4) at the time of diagnosis (4, 5). The 10-year survival rate for stage I melanoma patients is 90–97%, but only 3% for stage IV melanoma patients. Early detection and accurate assessment of the metastases remain the keys for improved outcome and disease-free survival. Unfortunately, the pattern of melanoma spread is often unpredictable, and conventional imaging with chest radiography, ultrasonography, computed tomography, and magnetic resonance imaging provides limited value for accurate staging and quantification of the disease burden (6, 7). Whole-body PET imaging with ^18^F-labeled fluorodeoxyglucose ([^18^F]FDG) has been shown to be superior to conventional imaging for detection of metastatic diseases, but it has not been shown to be useful for detecting small metastatic tumors (7, 8). Positive detection of nodal metastases requires nodal tumor involvement of more than 50% or capsular infiltration. Sub-centimeter pulmonary and hepatic metastases are frequently missed. Physiological uptake of FDG by the brain also limits its value in screening brain metastases. In an attempt to identify biomarkers of clinical utility, a large set of genes has been investigated for their abnormal expressions in melanoma (9-11). Potential biomarkers include p53, c-myc, CD44, Ki-67, Bcl-2, MITF, MMP2, p16, HIF2α, CXCR4, CEACAM1, p-Akt, β1 and β3 integrins, tPA, ICAM1, ephrin A1, β-catenin, P-cadherin, pleiotropin, PLK-1, and PUMA (9-11). Although these biomarkers offer the possibility of improved tumor staging through the molecular detection of microscopic metastases, these studies have been hampered by the failure of individual biomarkers to provide significant prognostic information beyond the current staging system.

Benzamide derivatives represent a versatile class of compounds used as agents for molecular imaging, as transporters for cytostatic agents, and as inhibitors for histone deacetylases (12). Since N-(2-diethylaminoethyl)-4-[^125^I]iodobenzamide ([^125^I]BZA) was first demonstrated to have high melanoma uptake, much effort has been made to further improve the affinity and pharmacological properties of this compound by modifying its structure such as using phenyl and amide substitutes (13, 14). Most benzamide derivatives possess the common structure element of Ph-CONH(CH_2_)_m_NR_2_ (m = 1,2), and they exhibit comparable properties such as high melanoma uptake, which is a positive attribute for potentially useful imaging agents (12). The exact mechanism for the high melanoma uptake has not been fully established, although direct melanin binding, involvement in the melanin biosynthesis pathway, and sigma receptor mediation have been proposed as the most likely mechanisms for different derivatives. Garg et al. developed a radiolabeled benzamide derivative, N-(2-diethylaminoethyl) 4-[^18^F]fluorobenzamide ([^18^F]-DAFBA), using the same structural motif of N-diethylaminoethyl-4-[^123^I]iodobenzamide (4-[^123^I]BZA) (1, 15). Garg et al. replaced the 4-iodo group of 4-[^123^I]BZA with a 4-fluoro group while keeping the remainder of the molecule unchanged. [^18^F]-DAFBA exhibited high melanoma uptake and low normal tissue retention. Their results suggest that [^18^F]-DAFBA could be a potentially useful probe to image melanoma. Ren et al. synthesized and tested the same agent with the name of ^18^F-FBZA as a PET tracer (2).

Benzamide Derivatives-Related Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Benzamide++AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=fluorobenzamide+and+PET)]

Garg et al. detailed the synthetic procedures of native DAFBA and [^18^F]-DAFBA (1). The native DAFBA was prepared as a high-performance liquid chromatography (HPLC) reference standard for the production of [^18^F]-DAFBA, and it was synthesized with the reaction of 4-fluorobenzoic acid in dichloromethane with triethylamine and ethyl chloroformate for 1 h at 0°C. This reaction mixture was further reacted with N,N-diethylethylenediamine for 2 h at room temperature. The desired DAFBA was obtained with 84% yield and 98% chemical purity after HPLC. The radiochemical synthesis of [^18^F]-DAFBA was accomplished by first synthesizing 4-[^18^F]fluorobenzoic acid followed by its coupling to N,N-diethylethylenediamine. The 4-[^18^F]fluorobenzoic acid was prepared via two separate routes. For the first route, 4-[^18^F]fluorobenzaldehyde was prepared first, followed by oxidation of the aldehyde group to the carboxylic acid group. With this route, the 4-[^18^F]fluorobenzoic acid was synthesized with a 72 ± 11% radiochemical yield. For the second route, 4-[^18^F]fluorobenzoic acid was prepared in two steps, first by preparing ethyl-[^18^F]fluorobenzoate followed by hydrolyzing the ester group to yield 4-[^18^F]fluorobenzoic acid without isolating the intermediate ethyl ester. With the second route, the radiochemical yield of 4-[^18^F]fluorobenzoic acid was 82 ± 8% (n = 11). The coupling of N-N-diethylethylenediamine to 4-[^18^F]fluorobenzoic acid was accomplished with 1-(3-dimethylaminopropyl)-3-ethylcarbodiimide hydrochloride as the coupling agent. After coupling and purification, [^18^F]-DAFBA was obtained with 54 ± 18% radiochemical yield, 97 ± 2% radiochemical purity, and >37 GBq (>1,000 mCi)/μmol specific activity. The overall synthesis time for [^18^F]-DAFBA, including HPLC purification and the final formulation, was 175 ± 15 min (n = 17). The radiochemical purity of [^18^F]-DAFBA remained >95% for up to 6 h after preparation of the product.

Ren et al. also described the synthesis of nonradioactive [^19^F]-DAFBA and radioactive [^18^F]-DAFBA under the names ^19^F-FBZA and ^18^F-FBZA, respectively (2). [^19^F]-DAFBA was synthesized in a one-step coupling reaction for 80 min at 50°C between N,N-diethylenediamine (DEDA) in dimethyl sulfoxide and N-succinimidyl-4-fluorobenzoate (SFB) in N,N'-diisopropylethylamine. After purification, the yield of [^19^F]-DAFBA was 70% and the measured molecular weight was 239.08 Da. Radiosynthesis of [^18^F]-DAFBA was achieved through coupling of ^18^F-SFB with the amino group of DEDA for 30 min at 50°C, followed by purification. The total radiosynthesis time for [^18^F]-DAFBA was 3 h, with an overall decay-corrected yield of 50% at the end of synthesis. The specific activity was estimated to be 132–166 GBq (3.57–4.49 Ci/µmol), and the radiochemical purity was >95%. The percentages of intact [^18^F]-DAFBA was 94.1%, 93.5%, 87.8%, and 85.1% at 30, 60, 120, and 150 min after incubation with mouse serum, respectively. Defluorination in mouse serum was not observed up to 150 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=fluorobenzamide+and+PET)]

Garg et al. analyzed the cell uptake of [^18^F]-DAFBA in B16F1 mouse melanoma cells (1). The [^18^F]-DAFBA uptake increased with increasing numbers of cultured cells, presenting an uptake of 5.60 ± 2.67% injected dose (ID) when 1 × 10^6^ cells/tube were incubated with ~200 kcpm of [^18^F]-DAFBA. The role of sigma receptors on the [^18^F]-DAFBA cell uptake was then analyzed with competitive binding assay. For sigma-1 receptor binding, the assay was performed using the guinea pig brain membrane and the specific ligand ^3^H-PENT. For sigma-2 receptor binding, the assay was performed using Sprague-Dawley rat liver membrane and the ligand ^3^H-DTG. The results showed that sigma receptors were not implicated in the cell uptake of [^18^F]-DAFBA. Because iodobenzamides with higher lipophilicity have been suggested to show better tumor uptake properties, and a log P_7.4_ of more than 1.4 is necessary for the enhanced tumor uptake characteristics, Garg et al. first calculated the log P value of [^18^F]-DAFBA to be 2.01. They then measured the partition coefficient of [^18^F]-DAFBA to be 1.7, a value similar to its calculated log P value. A higher lipophilicity (higher log P) may enhance tissue penetration to improve tumor uptake, but it would simultaneously increase the nonspecific uptake in target and nontarget tissues. It is essential to carefully balance the physicochemical parameters when designing new probes.

Ren et al. also analyzed the cell uptake of [^18^F]-DAFBA after 2 h incubation of 1 × 10^6^ B16F10 murine melanoma cells with 3.7 kBq (0.1 µCi) [^18^F]-DAFBA (2). Without pretreatment of the cells with L-tyrosine, the cell uptake after 2 h incubation was 0.49 ± 0.03% ID and 0.52 ± 0.1% ID at 4°C and 37°C, respectively. Pretreatment with L-tyrosine for 24 h significantly enhanced the cell uptake of [^18^F]-DAFBA at both 4°C and 37°C (P < 0.001). At 37°C, uptake by the tyrosine-stimulated cells peaked at 30 min (10.7 ± 0.8% ID), and the uptake remained at the level of 8.1 ± 1.9% ID at 2 h, an 18- to 25-fold increase compared with uptake by the nontreated B16F10 cells. Similar to the results obtained by Garg et al. (1), Ren et al. also showed that [^19^F]-DAFBA displayed a low affinity for both the sigma-1 receptor (inhibition constant, 8.90 µmol) and the sigma-2 receptor (inhibition constant, 0.12 mmol).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=fluorobenzamide+and+PET)]

Garg et al. first investigated the biodistribution of [^18^F]-DAFBA in ICR normal mice (n = 20) (1). In general, a low uptake was observed in most normal tissues over a 180-min study period. The kidneys and liver showed the highest uptake with 4.13 ± 0.68% ID/g for the kidneys and 3.12 ± 0.62% ID/g for the liver at 30 min after injection. The radioactivity rapidly washed out from the kidneys and liver, approaching the levels seen in other normal tissues at 180 min (liver, 1.12 ± 0.20% ID/g; kidney, 1.34 ± 0.36% ID/g). Similar results were observed for the lungs, presenting radioactivity levels of 1.75 ± 0.43% ID/g at 30 min and 0.49 ± 0.07% ID/g at 180 min after injection. The radioactivity in blood was quite low at all time points, presenting 0.78 ± 0.07% and 0.21 ± 0.03% ID/g at 30 and 180 min after injection, respectively.

Garg et al. then investigated the tumor uptake of [^18^F]-DAFBA in C57 mice bearing B16F1 melanoma tumor allografts (n = 20) (1). The [^18^F]-DAFBA accumulation in the tumor-bearing mice was quite similar to that observed in the ICR normal mice. Most normal tissues had a low accumulation. In the tumor, [^18^F]-DAFBA displayed a rapid and high uptake. The tumor uptake reached 7.00 ± 2.76% ID/g by 60 min and decreased only slightly by 180 min (5.80 ± 0.98% ID/g) with no statistical significance between the two time points (P > 0.2). The tumor uptake was also not dependent on the amount of radioactivity present in the blood pool (r = 0.32, P > 0.05). A high uptake in the tumor and low accumulation in the normal tissues resulted in a favorable tumor/normal tissue ratio. The tumor/blood ratio increased from 8.3 ± 3 at 60 min to 39 ± 12 at 180 min, a five-fold increase. Similarly, tumor/lung and tumor/muscle ratios were >20 at 180 min. [^18^F]-DAFBA crossed the blood–brain barrier within 30 min. After initial high uptake by the brain, the radioactivity rapidly decreased. The [^18^F]-DAFBA uptake in the normal brain was 2.02 ± 0.35% ID/g at 30 min and reduced to 0.29 ± 0.05% ID/g by 180 min, suggesting a low affinity of [^18^F]-DAFBA for normal brain tissue. Garg et al. concluded that rapid and high uptake of [^18^F]-DAFBA in tumor and low accumulation in normal tissues indicated its potential as a promising PET imaging probe to provide a high signal/noise ratio and an ability to clearly visualize tumors with low background signals (1). No blocking studies were reported.

Ren et al. performed biodistribution studies of [^18^F]-DAFBA in the subcutaneous and pulmonary metastasis models of B16F10 murine allografts as well as A375M and U87MG xenografts (n = 3 mice/group) (2). Amelanotic A375M human melanoma and U87MG human glioblastoma were used as control tumors. In the B16F10 subcutaneous tumor allografts (C57BL/6 mice), [^18^F]-DAFBA displayed a significant uptake being 6.47 ± 2.16% ID/g and 5.94 ± 1.83% ID/g at 1 h and 2 h after injection, respectively. The tumor/blood and tumor/muscle ratios reached 34.0 ± 13.2 and 23.3 ± 10.1 at 2 h after injection, respectively. In the A375M and U87MG mouse models (Nu/Foxn1 mice), however, the uptake in both A375M (0.75 ± 0.09% ID/g) and U87MG (0.56 ± 0.13% ID/g) xenografts was low, with tumor/blood ratios of 4.70 ± 0.78 and 3.57 ± 1.34 at 2 h after injection, respectively. For the B16F10 pulmonary metastasis model (C57BL/6 mice), animals were divided into two groups with 0.2 × 10^6^ cells injected for the first group and 0.4 × 10^6^ cells injected for the second group (n = 3 mice/group). The radioactivity in the lung with metastases reached 10.0 ± 3.92% ID/g for first group and 7.87 ± 3.56% ID/g for the second group at 2 h after injection. In the normal lung tissue, the probe accumulation was 0.99 ± 0.04% ID/g at 2 h after injection. The lung/blood ratios for the pulmonary metastasis model were 24.7 ± 13.5 and 38.9 ± 10.3 for the first and second groups, respectively. The lung/blood ratios at 2 h were 4.72 ± 0.46 and 4.23 ± 0.66 for the B16F10 subcutaneous model and control C57BL6 mice, respectively. Both absolute lung uptake and lung/blood ratio were significantly higher for the pulmonary metastasis model than for the subcutaneous model or for control C57BL/6 mice (P < 0.01). Small-animal PET imaging showed that the B16F10 tumors were clearly visualized at 1 h with a good tumor/background contrast, but A375M and U87MG tumors were not visualized well (n = 3 mice/group). B16F10 had a tumor uptake of 5.6 ± 1.2% ID/g, while A375M and U87MG had 0.86 ± 0.03% ID/g and 0.61 ± 0.04% ID/g (P < 0.01), respectively, suggesting specific binding of the [^18^F]-DAFBA to melanin containing tumors. Liver and kidney uptake was visualized in all animals. The lung with metastasis, compared with the normal lung, clearly showed a region of symmetric uptake greater than the background level in the chest. Normal lung uptake of the [^18^F]-DAFBA was 1.2 ± 0.2% ID/g, whereas uptake values of 10.2 ± 0.1% ID/g, 9.0 ± 0.4% ID/g, and 15.3 ± 1.1% ID/g were observed for lungs harboring metastases resulting from tumor doses of 0.2, 0.4, or 0.8 × 10^6^ B16F10 cells, respectively. The total number of metastases and the metastatic tumor volume in the lungs were not described.

Ren et al. also performed a comparative analysis of [^18^F]-DAFBA and ^18^F-FDG in C57BL/6 mice with B16F10 allografts (n = 3 mice for [^18^F]-DAFBA; n = 5 mice for ^18^F-FDG) (2). The results showed that the uptake levels for the two agents in the B16F10 tumors at 1 h were not significantly different. The lung uptake values were 7.61 ± 1.53% ID/g and 2.92 ± 0.40% ID/g for ^18^F-FDG and [^18^F]-DAFBA, respectively, suggesting much higher normal-lung uptake of the ^18^F-FDG (P < 0.01). Heart uptake of the ^18^F-FDG was also significantly higher than that of the [^18^F]-DAFBA (P < 0.01). However, liver uptake of the ^18^F-FDG was lower than that of the [^18^F]-DAFBA (P < 0.05).

Small-animal PET imaging of the B16F10 melanoma using [^18^F]-DAFBA or ^18^F-FDG showed that the two agents had different biodistribution patterns. High accumulation of the [^18^F]-DAFBA was observed in the tumor and liver, and [^18^F]-DAFBA was washed out through the kidneys. While high accumulation of the ^18^F-FDG was observed in the heart, eyes (Harderian glands), and tumor, radioactivity in the liver was low. The tumor uptake was 5.6 ± 1.2% ID/g for [^18^F]-DAFBA and 6.31 ± 0.61% ID/g for ^18^F-FDG (P > 0.05). PET/computed tomography fusion images clearly demonstrated the tumor anatomy and specific tumor uptake of both probes. On the basis of their results, Ren et al. also concluded that [^18^F]-DAFBA specifically targets primary and metastatic melanotic melanoma lesions with high tumor uptake and may have translational potential (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Garg, S., K. Kothari, S.R. Thopate, A.K. Doke, and P.K. Garg, Design, Synthesis, and Preliminary in Vitro and in Vivo Evaluation of N-(2-diethylaminoethyl)-4-[(18)F]fluorobenzamide ([(18)F]-DAFBA): A Novel Potential PET Probe to Image Melanoma Tumors. Bioconjug Chem, 2009
2 Ren G., Miao Z., Liu H., Jiang L., Limpa-Amara N., Mahmood A., Gambhir S.S., Cheng Z. (2009). Melanin-targeted preclinical PET imaging of melanoma metastasis. J Nucl Med.
3 Lens M. (2008). Current clinical overview of cutaneous melanoma. Br J Nurs.
4 Mohr P., Eggermont A.M., Hauschild A., Buzaid A. (2009). Staging of cutaneous melanoma. Ann Oncol.
5 McLoughlin J.M., Zager J.S., Sondak V.K., Berk L.B. (2008). Treatment options for limited or symptomatic metastatic melanoma. Cancer Control.
6 Choi E.A., Gershenwald J.E. (2007). Imaging studies in patients with melanoma. Surg Oncol Clin N Am.
7 Kochhar, R., H. Ali, S. Mak, and P. Manoharan, Metastatic cutaneous malignant melanoma: spectrum of imaging findings and the role of multimodality imaging. J Med Imaging Radiat Oncol, 200953(5): p. 467-78; quiz 478-9.
8 Essner R., Belhocine T., Scott A.M., Even-Sapir E. (2006). Novel imaging techniques in melanoma. Surg Oncol Clin N Am.
9 Gogas H., Eggermont A.M., Hauschild A., Hersey P., Mohr P., Schadendorf D., Spatz A., Dummer R. (2009). Biomarkers in melanoma. Ann Oncol.
10 Larson A.R., Konat E., Alani R.M. (2009). Melanoma biomarkers: current status and vision for the future. Nat Clin Pract Oncol.
11 Rother J., Jones D. (2009). Molecular markers of tumor progression in melanoma. Curr Genomics.
12 Oltmanns D., Eisenhut M., Mier W., Haberkorn U. (2009). Benzamides as melanotropic carriers for radioisotopes, metals, cytotoxic agents and as enzyme inhibitors. Curr Med Chem.
13 Michelot J.M., Moreau M.F., Labarre P.G., Madelmont J.C., Veyre A.J., Papon J.M., Parry D.F., Bonafous J.F., Boire J.Y., Desplanches G.G., et al. (1991). Synthesis and evaluation of new iodine-125 radiopharmaceuticals as potential tracers for malignant melanoma. J Nucl Med.
14 Mansard S., Papon J., Moreau M.F., Miot-Noirault E., Labarre P., Bayle M., Veyre A., Madelmont J.C., Moins N. (2005). Uptake in melanoma cells of N-(2-diethylaminoethyl)-2-iodobenzamide (BZA2), an imaging agent for melanoma staging: relation to pigmentation. Nucl Med Biol.
15 Sillaire-Houtmann I., Bonafous J., Veyre A., Mestas D., D'Incan M., Moins N., Kemeny J.L., Chossat F., Bacin F. (2004). J Fr Ophtalmol.